# T84.66 Anti-CEA diabody-GSTSGSGKPGSGEGSTSG-Renilla luciferase

Chemical name: | T84.66 Anti-CEA diabody-GSTSGSGKPGSGEGSTSG-Renilla luciferase
Abbreviated name: | Db-18-Rluc8
Synonym:
Agent category: | Antibody
Target: | Carcinoembryonic antigen (CEA)
Target category: | Antigen
Method of detection: | Optical Imaging
Source of signal/contrast: | Luciferin
Activation: | Yes
Studies: | - In vitro; - Rodents | No structure is currently available in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=diabody + Rluc8)]

Carcinoembryonic antigen (CEA) is a highly glycosylated protein with a molecular mass of 180 kDa that belongs to the immunoglobin supergene family (1). CEA contains ~60% carbohydrate and a protein portion of 668 amino acids. As a common human tumor antigen, CEA is overexpressed on >80% of colorectal, pancreatic, breast, non-small cell lung, and medullary cancers, and on >70% of gastric, invasive cervical, endometrial, urinary bladder, and head/neck cancers (2). A variety of antibodies have been developed to target CEA. For example, T84.66 is a murine monoclonal antibody with a molecular mass of 150 kDa with exceptionally high affinity (2.6 × 10^10^ M^-1^) for the α_3_β_3_ epitope on the CEA (2, 3). T84.66 has been used to quantify CEA expression in immunohistological staining and in in vivo imaging. The T84.66 diabody is a recombinant fragment of the antibody that comprises two identical single chain variable (scFv) regions (4). Each scFv consists of a V_L_ domain of 107 amino acids, a peptide linker of 8 amino acids (GGGSGGGG), and a V_H_ domain of 112 amino acids. The two scFvs associate asymmetrically to form a stable diabody (scFv dimer) with a molecular mass of 55 kDa. T84.66 diabody retains the high avidity of T84.66 via its bivalent binding. The small size of the diabody allows for rapid in vivo targeting in imaging and therapeutic applications.

Renilla luciferase (Rluc) is a 36-kDa enzyme protein extracted from a bioluminescent soft coral (sea pansy (Renilla reniformis)) (5). Rluc can catalyze emission of light from substrates, i.e., the oxidation of coelenterazine to coelenteramide generates a green fluorescence (535–550 nm) (6). Unlike the luciferase obtained from the firefly (Fluc), the Rluc oxidation process does not depend on adenosine-5'-triphosphate (7). Thus, Rluc is suitable for use as an in vivo bioluminescent tag, i.e., Rluc has been reported as a marker of gene expression in various cells and as a reporter gene or cell tag for in vivo imaging (5). Rluc8 is a variant of Rluc that contains amino acid substitution at the following eight locations: A55T, C124A, S130A, K136R, A143M, M185V, M253L, and S287L (5). These substitutions enhance the enzymatic activity stability of the molecule (>200 h) and increase the light emission as much as four-fold. The small size of Rluc makes it suitable for fusion with other proteins to generate specifically labeled proteins for imaging applications.

T84.66 Anti-CEA diabody-GSTSGSGKPGSGEGSTSG-Renilla luciferase (Db-18-Rluc8) is an optical agent used for imaging CEA (5). Db-18-Rluc8 contains three components: a T84.66 diabody for targeting CEA, an Rluc8 for catalyzing the coelenterazine substrate to emit light for optical detection, and a peptide linker of 18 amino acids to connect the diabody portion and the luciferase portion. The three components were assembled via protein fusion. Db-18-Rluc8 allows for localization of CEA-positive tumors in the living animal.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(diabody + Rluc8)+AND+synthesis%0D%0A)]

Venisnik et al. briefly described the preparation of Db-18-Rluc8 (5). The gene encoding the T84.66 anti-CEA diabody was fused to the Rluc8 gene from phRL-CMV vector via slice overlap polymerase chain reaction (PCR). During this process, a linker of 18 amino acids (GSTSGSGKPGSGEGSTSG) was inserted between the diabody and the Rluc8. The obtained Db-18-Rluc8 gene was inserted into the bacterial expression plasmid pKKtac using HindIII and EcoRI sites, and a pelB leader sequence was included to facilitate bacterial expression and protein purification. The fused protein Db-18-Rluc8 was extracted from periplasmic secretion and purified with Ni-NTA chromatography. Db-18-Rluc8 protein also was obtained from expression in NS0 murine myeloma cells (5), which was transfected via electroporation with the Db-18-Rluc8 gene in a pFF12 expression vector.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(diabody + Rluc8)+AND+%22in+vitro%22)]

The stability of the luminescence activity produced by Db-18-Rluc8 was examined in mouse serum. The half-life of the enzymatic activity was found to be >200 h with a Michaelis constant of 1.6 μM for catalyzing coelenterazine. The bimolecular functionality of Db-18-Rluc8 was evaluated on the basis of its ability to bind CEA (the diabody portion) and its ability to emit light (the luciferase portion). Db-18-Rluc8 appeared to bind N-A3 protein, a recombinant CEA fragment, and to emit light by oxidizing coelenterazine. The binding to CEA was further examined with flow cytometry analysis of CEA-expressing human LS174T colon carcinoma cells. After incubation for 45 min, 83.8% LS174T cells were stained positive for Db-18-Rluc8, similar to the proportion stained with the anti-CEA antibody (T84.1 murine IgG_1_).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(diabody + Rluc8) +AND++rodentia)]

The specificity of Db-18-Rluc8 binding to tumor was examined in vivo (5). Athymic mice (n = 7) bearing 140–200 μg LS174T tumors (CEA-positive) were intravenously injected with 100 μl of Db-18-Rluc8 solution (17 μg of total protein, 9.1 × 10^8^ relative light units (RLU)). At 2, 4, 6, 8, and 24 h after injection, optical images were acquired with the cooled charge-coupled device camera immediately after intravenous injection of coelenterazine (0.7 mg/kg). Optical signal became observable at 2 h and increased over time. The tumor signal to tissue background ratio (S/B) peaked at 6 h (6.0 ± 0.8). At 24 h, the target was still visible with S/B ratio of 2.8 ± 0.7. Athymic mice (n = 7) bearing 140–200 mg C6 rat glioma xenografts (CEA-negative) were examined as a control. The S/B ratio in the C6 tumors was 1.0 ± 0.1 at all time points, which was significantly lower than that in the LS174T tumors. Two additional control experiments were performed, including assessment the uptake of luciferase or coelenterazine in tumors and tissues. No specific targeting was found in either case. The specificity and dynamics of binding were further examined in vivo with ^124^I-labeled Db-18-Rluc8 (5). Athymic mice (n = 4) bearing LS174T tumors (120–140 mg) or C6 rat glioma xenografts (45–100 mg) were injected intravenously with 140–150 μCi ^124^I-labeled Db-18-Rluc8 solution. Positron emission tomography (PET) was performed 4 or 21 h after injection. At 4 h, the S/B ratio in the LS174T tumor was 3.8 ± 0.8 compared with 1.2 ± 0.3 in the C6 tumors. At 21 h, the S/B ratio increased significantly to 18.0 ± 5.3 in the LS174T tumor but retained the same level in the C6 tumor (1.6 ± 0.3). After collecting the PET images at 21 h, the animals were euthanized and tissues were harvested for quantification of uptake. Accumulation of ^124^I appeared to be significantly high in the LS174T tumor (12.9 ± 1.8% ID/g) compared with that in the C6 tumor (1.7 ± 0.40% ID/g) and that in the tissue (<0.8% ID/g).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(diabody + Rluc8) +AND+(primate+non+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(diabody + Rluc8) +AND+human)]

No publication is currently available.

### NIH Support

GM 08652, CA 43904, CA 92865, CA 082214, CA 16042

## References

1 Thomas P., Toth C.A., Saini K.S., Jessup J.M., Steele G. (1990). The structure, metabolism and function of the carcinoembryonic antigen gene family. Biochim Biophys Acta.
2 Blumenthal R.D. (2004). Technology evaluation: cT84.66, City of Hope. Curr Opin Mol Ther.
3 Neumaier M., Shively L., Chen F.S., Gaida F.J., Ilgen C., Paxton R.J., Shively J.E., Riggs A.D. (1990). Cloning of the genes for T84.66, an antibody that has a high specificity and affinity for carcinoembryonic antigen, and expression of chimeric human/mouse T84.66 genes in myeloma and Chinese hamster ovary cells. Cancer Res.
4 Carmichael J.A., Power B.E., Garrett T.P., Yazaki P.J., Shively J.E., Raubischek A.A., Wu A.M., Hudson P.J. (2003). The crystal structure of an anti-CEA scFv diabody assembled from T84.66 scFvs in V(L)-to-V(H) orientation: implications for diabody flexibility. J Mol Biol.
5 Venisnik K.M., Olafsen T., Loening A.M., Iyer M., Gambhir S.S., Wu A.M. (2006). Bifunctional antibody-Renilla luciferase fusion protein for in vivo optical detection of tumors. Protein Eng Des Sel.
6 Loening A.M., Wu A.M., Gambhir S.S. (2007). Red-shifted Renilla reniformis luciferase variants for imaging in living subjects. Nat Methods.
7 Loening A.M., Fenn T.D., Wu A.M., Gambhir S.S. (2006). Consensus guided mutagenesis of Renilla luciferase yields enhanced stability and light output. Protein Eng Des Sel.